# Radioiodinated anti-CD105 MAEND3 monoclonal antibody

Chemical name: | Radioiodinated Anti-CD-105 MAEDND3 monoclonal antibody
Abbreviated name: | ^125^I-MAEND3 MAb
Synonym: | Radioiodinated anti-endoglin MAb, ^125^I-anti-endoglin MAb, ^125^I-anti-EDG MAb, ^125^I-anti-TGF-ß binding receptor MAb
Agent Category: | Antibody
Target: | Endoglin (CD105, EDG)
Target Category: | Antibody to antigen binding
Method of detection: | Single-photon emission computed tomography (SPECT), Gamma planar imaging
Source of signal/ contrast: | ^125^I
Activation: | No
Studies: | - In vitro; - Non-primate non-rodent mammals | Click on protein (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=protein&val=4557555), nucleotide (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=nucleotide&val=10862690) (RefSeq), and gene (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?db=gene&cmd=Retrieve&dopt=full_report&list_uids=2022) for more information about CD105

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=125I-anti-endoglin+antibody+OR+MAEND3+monoclonal+antibody)]

Radioiodinated-Anti-CD105 MAEND3 monoclonal antibody (Radiodinated-MAEND3 MAb), which is formed by the radioiodination of an intact MAEND3 MAb against the antigen endoglin (cluster of differentiation 105 (CD105)), an accessory component of the receptor complex of transforming growth factor-β (TGF-β), has been developed for gamma imaging of tumor neovasculature (1). ^125^I was used in the investigation, and it is a low-energy gamma emitter with a long physical half-life (t_½_) of 60 days.

Because tumor growth and metastasis largely depend on angiogenesis, targeting of tumor vasculature is a promising strategy for cancer imaging and therapy (2). TGF-β is a pleiotropic cytokine that modulates angiogenesis, vascular remodeling, and tumor progression. Three isoforms of TGF-β, β_1_ to β_3_, have been identified. TGF-β_1_ appears to inhibit proliferation and migration of endothelial cells and their ability to form capillaries. CD105 (EDG) is a homodimeric cell membrane glycoprotein of 180 kDa, and it is a component of the TGF-β receptor complex that binds TGF-β_1_ and TGF-β_3_ with high affinity. CD105 is critical for correct blood vessel development. The expression of CD105 on different cells affects cellular response to TGF-β_1_. CD105 is overexpressed in proliferating endothelial cells of tumor vessels, and they prevent TGF-β_1_ inhibition of cellular proliferation (3, 4). Two isoforms of CD105, L and S, have been identified. L-CD105 is a protein of 633 amino acids and is expressed predominantly on endothelial cells. The molecular weight of CD105 is ~180,000 with disulfide-linked subunits of 95,000. The CD105 gene in humans has been mapped to chromosome 9q34→qter.

Radiolabeled MAbs have been developed for both the diagnosis and treatment of tumors (5-7). Quiescent human endothelial cells express CD105 only weakly, but the expression of CD105 is strongly up-regulated on the endothelium of tumor tissues undergoing angiogenesis (4). The high level of expressed CD105 (up to 10^6^ molecules/proliferating cell) appears to be ideal for in vivo imaging and therapy. Tabata et al. (3) first investigated tumor targeting with ^125^I-labeled anti-CD105 MAbs in human breast tumor-bearing severe combined immune deficiency mice. The results showed the possible usefulness of antiangiogenic radioimmunotherapy with radiolabeled anti-CD105 MAbs. Anti-CD105 MAbs labeled with photon emitters can be used for tumor imaging. Fonsatti et al. (1) showed that a ^125^I-labeled anti-CD105 MAb (MAEND3) could efficiently image spontaneous mammary adenocarcinomas in two dogs. ^125^I does not have the proper physical properties and is not an ideal radionuclide for imaging, but other radioactive iodines (^131^I, ^123^I) with better imaging properties are available.

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=(125I-anti-endoglin+antibody+OR+MAEND3+monoclonal+antibody)+AND+synthesis)]

Fonsatti et al. (1) developed the antihuman CD105 MAb, MAEND3, which cross-reacted with rat CD105. Pichuantes et al. (8) reported the production of MAED3 MAb that was able to bind to CD105. They also showed that the MAb bound to a region of 54 amino acids encoded mostly by exon 7. Iodination with ^125^I was performed by the IodoGen (1,3,4,6-tetrachloro-3,6-diphenylglycoluril) method as follows: 1 mg of MAEND3 and 50 MBq (1.35 mCi) were mixed in an IodoGen-coated vial. AG1-X-8 resin was added to absorb the free IodoGen and stop the reaction. The specific activity obtained was 37 MBq (1 mCi)/mg, or 5.6 GBq (0.15 Ci)/μmol based on a molecular weight of 150,000 for the intact MAb. The radiochemical yield and purity were not reported.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=(125I-anti-endoglin+antibody+OR+MAEND3+monoclonal+antibody)+AND+in+vitro)]

Fonsatti et al. (1) performed in vitro indirect immunoperoxidase stain (IIF) with the unlabeled MAEND3 MAb on human breast cancer cells (SK-BR-3, DAL, and MCF7) and human umbilical vein endothelial cells (HUVECs). Immunochemistry and flow cytometry showed strong CD105 expression in HUVECs but weak or no expression in breast cancer cells. The IIF staining with MAEND3 MAB was consistent with the level of CD105 expressions on these cell lines. Infiltrating ductal breast adenocarcinoma tissue samples were obtained from surgical biopsies of patients, MAEND3 MAb rarely and heterogeneously stained neoplastic cells in 5 of 30 infiltrating ductal breast adenocarcinomas, but blood vessel endothelia were strongly stained in all tumor samples.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=(125I-anti-endoglin+antibody+OR+MAEND3+monoclonal+antibody)+AND+in+vitro)]

No publication is currently available.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=(125I-anti-endoglin+antibody+OR+MAEND3+monoclonal+antibody)+AND+(dog+OR+rabbit+OR+pig+OR+sheep))]

Fonsatti et al. (1) conducted imaging studies of ^125^I-labeled anti-CD105 MAb (MAEND3) in two Beagle dogs bearing a spontaneous canine mammary carcinoma. The dogs were injected with 18 MBq (0.49 mCi) of ^125^I-MAEND3. Imaging was performed 8 h after injection, and it showed that tumor radioactivity uptake was rapid and intense. The tumor/background ratios were 8.2:1 and 9.3:1 for the two dogs. Radioactivity was also detected in the urinary bladders. Stomach and heart radioactivities were identified in only one dog. These organs were outside the imaging field in the second dog. Surgical excision of mammary neoplasm was performed 10 days after imaging, and histologic diagnosis of grade II ductal mammary adenocarcinoma was confirmed.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=(125I-anti-endoglin+antibody+OR+MAEND3+monoclonal+antibody)+AND+(primate+NOT+human))]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=(125I-anti-endoglin+antibody+OR+MAEND3+monoclonal+antibody)+AND+human)]

No publication is currently available.

## References

1 Fonsatti E., Jekunen A.P., Kairemo K.J., Coral S., Snellman M., Nicotra M.R., Natali P.G., Altomonte M., Maio M. (2000). Endoglin is a suitable target for efficient imaging of solid tumors: in vivo evidence in a canine mammary carcinoma model. Clin Cancer Res.
2 Fonsatti E., Altomonte M., Arslan P., Maio M. (2003). Endoglin (CD105): a target for anti-angiogenetic cancer therapy. Curr Drug Targets.
3 Tabata M., Kondo M., Haruta Y., Seon B.K. (1999). Antiangiogenic radioimmunotherapy of human solid tumors in SCID mice using (125)I-labeled anti-endoglin monoclonal antibodies. Int J Cancer.
4 Bredow S., Lewin M., Hofmann B., Marecos E., Weissleder R. (2000). Imaging of tumour neovasculature by targeting the TGF-beta binding receptor endoglin. Eur J Cancer.
5 Wu A.M., Senter P.D. (2005). Arming antibodies: prospects and challenges for immunoconjugates. Nat Biotechnol.
6 Milenic D.E., Brechbiel M.W. (2004). Targeting of radio-isotopes for cancer therapy. Cancer Biol Ther.
7 Kowalsky R.J., Falen S.W. (2004). Radiopharmaceutcals in nuclear pharmacy and nuclear medicine. Second ed. , Washington, D.C.: APhA. 733-752.
8 Pichuantes S., Vera S., Bourdeau A., Pece N., Kumar S., Wayner E.A., Letarte M. (1997). Mapping epitopes to distinct regions of the extracellular domain of endoglin using bacterially expressed recombinant fragments. Tissue Antigens.